# [^18^F]FB-NH-mini-PEG-E{E[c(RGDyK)]_2_}_2_

Chemical name: | [^18^F]FB-NH-mini-PEG-E{E(c(RGDyK)]_2_}_2_
Abbreviated name: | [^18^F]FPRGD4
Synonym: | ^18^F-PEG-RGD, ^18^F-labeled PEGylated tetrameric RGD peptide
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal /contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F-FPRGD4+OR+(18F-labeled+PEGylated+tetrameric+RGD+peptide))]

[^18^F]FB-NH-mini-PEG-E{E[c(RGDyK)]_2_}_2_ ([^18^F]FPRGD4) is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) of tumor vasculature and angiogenesis (1). ^18^F is a positron emitter with a physical half-life (t_½_) of 110 min.

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature.

Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7). Various RGD peptides in both linear and cyclic forms (RGDfK or RGDyK) have been developed for in vivo binding to integrin α_v_β_3_ (8). To improve the pharmacokinetics and tumor retention of the radiolabeled peptide, a dimer analog was synthesized as [^18^F]FB-[c(RGDyK)]_2_, which showed improved tumor localization and predominant renal excretion (9). Alternatively, Chen et al. (10) modified c(RGDyK) with monofunctional methoxy-polyethylene glycol (mPEG; molecular weight = 2,000 kDa) and showed that the modified PEGylated RGD peptide had faster blood clearance, lower kidney uptake, and prolonged tumor uptake. Using the same strategy, Chen et al. (11) inserted a heterofunctional PEG (molecular weight = 3,400 kDa) molecule between the [^18^F]fluorobenzoyl component and the RGD peptide to produce [^18^F]FB-PEG-c(RGDyK) for imaging of brain tumor angiogenesis. The PEGylated [^18^F]FB-c(RGDyK) analog appeared to improve tumor retention and in vivo kinetics compared with [^18^F]FB-c(RGDyK). These improvements might be attributed to a number of possible causes that include shielding of antigenic and immunogenic epitopes, shielding receptor-mediated uptake by the reticuloendothelial systems, preventing the recognition and degradation by proteolytic enzymes, and increasing the apparent size of the peptide. Wu et al. (12) reported that a multimeric RGD peptide with more than two repeating cyclic RGD units would further enhance the affinity of the receptor−ligand interactions through the phenomenon of a polyvalency effect. However, the attempt of synthesis of 18F-labeled tetrameric RGDyK peptiode (^18^F-FRGD4) proved to be difficult and gave very low yield (<2%) because of increased molecular size and steric hindrance (1). On the basis of these observations, Wu et al. (1) inserted a mini-PEG linker to improve the labeling yield and successfully prepared [^18^F]FPRGD4 by radiolabeling PEGylated tetrameric RGD peptide with reasonable yield. The in vivo kinetics of this PEGylated probe was studied in three different tumor models.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(18F-FPRGD4)+OR+(18F-labeled+PEGylated+tetrameric+RGD+peptide))]

Wu et al. (12) reported the preparation of cyclic RGD peptide tetramer E{E[c(RGDyK)]_2_}_2_ (RGD4) from the cyclic RGD dimer E[c(RGDyK)]_2_. RGD4 was then used to prepare NH_2_-Mini-PEG-E{E[c(RGDyK)]_2_}_2_ (PRGD4) (1). Briefly, Boc-11-amino-3,6,9-trioxaundecanoic acid (Boc-NH-mini-PEG-OOH) was mixed with N,N-diisopropylethylamine and O-(N-succinimidyl)-1,1,3,3-tetramethyl-uronium tetrafluoroborate (1). The reaction mixture was stirred at room temperature for 0.5 h. RGD4 in N,N-dimethylformamide was added to the mixture and stirred at room temperature for 2 h to produce Boc-NH-mini-PEG-E{E[c(RGDyK)]_2_}_2_. The yield was 60%. The Boc-group was then removed by treatment with trifluoroacetic acid (TFA) for 5 min at room temperature to yield PRGD4. PRGD4 was purified by high-performance liquid chromatography (HPLC) for radiolabeling. The identify of PRGD4 was confirmed by matrix-assisted laser desorption/ionization mass spectrometry with m/z 3,001.0 for [MH]^+^ (the calculated molecular weight of C_131_H_194_N_40_O_42_ = 3,001.1).

The purified product of PRGD4 was labeled with ^18^F by coupling with N-succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) (1, 13). The synthesis was conducted with a commercial synthesis module. The total synthesis time was ~100 min and the decay-corrected yield was 67 ± 11% (n = 10). The purified [^18^F]SFB was added to PRGD4 in dimethyl sulfoxide with DIPEA. This peptide mixture was incubated at 60ºC for 30 min. The final product was then diluted with 1% TFA in water before purified by semipreparative HPLC to yield [^18^F]FPRGD4. The decay-corrected radiochemical yield based on [^18^F]SFB was 22.0 ± 0.8% (n = 4). Analytical HPLC showed that the radiochemical purity was >99%. The specific activity was ~100–200 GBq/μmol (2.7-5.4 Ci/μmol) based on [^18^F]SFB. Starting from ^18^F-F^–^, the total synthesis time of [^18^F]FPRGD4 was ~180 min (including HPLC purification), and the overall decay-corrected yield was 15 ± 4%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((18F-FPRGD4)+OR+(18F-labeled+PEGylated+tetrameric+RGD+peptide))+AND+in+vitro)]

The octanol-water partition coefficient (log P) of [^18^F]FPRGD4 was determined to be –2.67 ± 0.22 with the use of phosphate-buffered saline and octanol (1). Wu et al. (1) conducted an in vitro cell (U87MG human glioblastoma) integrin receptor-binding assays with [^18^F]FPRGD4 by using ^125^I-echistatin (integrin α_v_β_3_ specific) in displacement studies. The 50% inhibitory concentration IC_50_ for [^18^F]FPRGD4 was 37.7 ± 7.0 nM (n = 3). In comparison, the IC_50_ values for RGD4 and PRGD4 were 39.1 ± 5.5 and 46.5 ± 5.3, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((18F-FPRGD4)+OR+(18F-labeled+PEGylated+tetrameric+RGD+peptide))+AND+rodentia)]

MicroPET imaging of 3.7 MBq (100 μCi) [^18^F]FPRGD4 in nude mice (n = 3) bearing the s.c. U87MG tumor (100-300 mm^3^) as early as 5 min clearly visualized the tumor with a high contrast to contralateral background (1). The radiolabeled peptide was cleared mainly through the kidneys with some hepatic clearance. Using the region-of-interest (ROI) technique, the tumor radioactivity levels (% ID/g) were calculated to be 9.87 ± 0.10 (5 min), 7.80 ± 0.14 (30 min), 6.40 ± 0.27 (60 min), 5.39 ± 0.14 (120 min), and 4.82 ± 0.22 (180 min). When a blocking dose of 10 mg/kg c(RGDyK) was given, more than 80% of the tumor radioactivity was inhibited. Other major organ radioactivity levels were also reduced.

MicroPET imaging of 3.7 MBq (100 μCi) [^18^F]FPRGD4 was conducted in nude mice (n = 3) bearing the MDA-MB-435 tumor (orthotopic injection into the left mammary fat pad) which had lower integrin expression level than the U87MG tumor (1). The ROI tumor radioactivity levels (% ID/g) were lower that those of U87MG model with 5.07 ± 0.18 (30 min), 4.53 ± 0.36 (60 min), and 3.38 ± 0.48 (150 min). MicroPET imaging of 3.7 MBq (100 μCi) [^18^F]FPRGD4 was also performed in a spontaneous murine mammary carcinoma model grown in c-neu onomice (n = 3) (1). The ROI tumor radioactivity levels (% ID/g) were lower that those of U87MG model with 4.22 ± 0.18 (30 min), 3.56 ± 0.36 (60 min), and 2.36 ± 0.40 (150 min). Immunofluorescence staining of frozen tissue slices from c-neu oncomice confirmed the expression of β_3_-integrin in both tumor cells and endothelial cells of the murine mammary carcinoma (1). β_3_-integrin was also detected in the liver, lung, kidneys, and glomerulus. No significant difference in organ distribution of [^18^F]FPRGD4 was observed among all three animal models. In a control study, microPET imaging of 3.7 MBq (100 μCi) [^18^F]FPRGD4 in nude mice (n = 3) bearing an integrin-negative s.c. DU145 tumor. The ROI tumor radioactivity levels (%ID/g) were significantly lower with 1.44 ± 0.34 (30 min) and 0.93 ± 0.13 (60 min) (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((18F-FPRGD4)+OR+(18F-labeled+PEGylated+tetrameric+RGD+peptide))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((18F-FPRGD4)+OR+(18F-labeled+PEGylated+tetrameric+RGD+peptide))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((18F-FPRGD4)+OR+(18F-labeled+PEGylated+tetrameric+RGD+peptide))AND+human)]

No publication is currently available.

## NIH Support

NIH NIBIB R21 EB001785, NCI CA102123, P50 CA114747, U54 CA119367, R24 CA93862.

## References

1 Wu Z., Li Z.B., Chen K., Cai W., He L., Chin F.T., Li F., Chen X. (2007). microPET of tumor integrin alphavbeta3 expression using 18F-labeled PEGylated tetrameric RGD peptide (18F-FPRGD4). J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Chen X., Tohme M., Park R., Hou Y., Bading J.R., Conti P.S. (2004). Micro-PET imaging of alphavbeta3-integrin expression with 18F-labeled dimeric RGD peptide. Mol Imaging.
10 Chen X., Park R., Shahinian A.H., Bading J.R., Conti P.S. (2004). Pharmacokinetics and tumor retention of 125I-labeled RGD peptide are improved by PEGylation. Nucl Med Biol.
11 Chen X., Park R., Hou Y., Khankaldyyan V., Gonzales-Gomez I., Tohme M., Bading J.R., Laug W.E., Conti P.S. (2004). MicroPET imaging of brain tumor angiogenesis with 18F-labeled PEGylated RGD peptide. Eur J Nucl Med Mol Imaging.
12 Wu Y., Zhang X., Xiong Z., Cheng Z., Fisher D.R., Liu S., Gambhir S.S., Chen X. (2005). microPET imaging of glioma integrin {alpha}v{beta}3 expression using (64)Cu-labeled tetrameric RGD peptide. J Nucl Med.
13 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.